# Lactoferrin-conjugated poly(ethylene glycol)-coated Fe_3_O_4_ nanoparticles

Chemical name: | Lactoferrin-conjugated poly(ethylene glycol)-coated Fe_3_O_4_ nanoparticles
Abbreviated name: | Fe_3_O_4_-Lf
Synonym:
Agent Category: | Nanoparticles
Target: | Lactoferrin receptors
Target Category: | Receptors
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Fe_3_O_4_
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=BBB%20and%20review%20and%20delivery)]

The lactoferrin (Lf)-conjugated poly(ethylene glycol) (PEG)-coated Fe_3_O_4_ nanoparticles, abbreviated as Fe_3_O_4_-Lf, was synthesized by Qiao et al. for use as a contrast agent for magnetic resonance imaging (MRI) of the brain (1). As a ligand, Lf acts to enhance the blood–brain barrier (BBB) penetration and Lf receptor-targeting of Fe_3_O_4_-Lf.

BBB is composed of tight junction-sealed brain capillary endothelial cells (BCECs) and supporting pericytes and astrocytic endfeet (2). Exogenous compounds are prevented by the BBB from reaching the brain by passive transport or through the paracellular route (3). Because many proteins including Lf could effectively cross the BBB through transcytosis, an active transport mechanism of BCECs, this mechanism has been actively used to design brain-targeted delivery systems for targeted imaging and therapy of neurological diseases (4, 5).

Mammalian Lf is a cationic iron-binding glycoprotein (80 kDa), and its receptor expresses on the endothelial cells of BBB (6). Upon binding with its receptor, Lf could cross the BBB through receptor-mediated transcytosis (5). The transport of Lf across the BBB is unidirectional, from the apical side to the basolateral side, with no apparent intraendothelial degradation (1, 7). Studies with membrane preparations of mouse brains have shown that the Lf receptor in the BCECs has two classes of binding sites: a high-affinity site that has a dissociation constant (K_d_) of 10.61 nM and a B_max_ of 410 fmol bound/µg protein; and a low-affinity site that has a K_d_ of 2,228 nM and a B_max_ of 51,641 fmol bound/µg protein (5). The plasma concentration of endogenous Lf (~5 nM) is lower than the K_d_ of Lf receptors in the BBB, which avoids the competitive inhibition of endogenous Lf to exogenous Lf-conjugated agents (1). Lf receptor has also been shown to be overexpressed in various tumors including brain glioma (8). Because of these features, Lf has been applied as a ligand in designing brain-targeted delivery systems.

Xie et al. conjugated Lf to superparamagnetic iron oxide nanoparticles (SPIONs) to develop the contrast agent Lf-SPION (8), while Qiao et al. developed the agent Fe_3_O_4_-Lf by conjugating Lf to Fe_3_O_4_ nanoparticles through PEG (1). For the former agent, Lf was designed to target Lf-SPIONs to tumors expressing the Lf receptor. For the latter agent, Lf served to enhance the BBB-penetrating ability of Fe_3_O_4_-Lf by targeting Lf receptors expressed in the BCECs. Studies with the two agents showed that Lf-SPIONs were able to effectively enhance the glioma contrast, and Fe_3_O_4_-Lf could effectively penetrate the BBB in healthy rats because of the conjugation of Lf (1, 8). This chapter summarizes the data obtained by Qiao et al. with Fe_3_O_4_-Lf.

### Related Resource Links:

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=lactoferrin) and protein (http://www.ncbi.nlm.nih.gov/protein?term=lactoferrin) of lactoferrin

Protein (http://www.ncbi.nlm.nih.gov/protein?term=lactoferrin%20receptor) of lactoferrin receptor

Lactoferrin-related clinical trials (http://clinicaltrials.gov/ct2/results?term=lactoferrin&Search=Search) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=BBB%20and%20delivery%20and%20qiao)]

Qiao et al. described the synthesis of Fe_3_O_4_-Lf in detail (1). Briefly, the PEG-coated Fe_3_O_4_ nanoparticles were synthesized with a “one-pot” synthetic reaction of Fe(acac)_3_, oleylamine, and HOOC-PEG-COOH in the diphenyl ether solution. Ether was then used to precipitate and purify the Fe_3_O_4_ nanocrystal. The final product, PEG-coated Fe_3_O_4_, was formulated in either Milli-Q water or phosphate-buffered saline.

The average size of PEG-coated Fe_3_O_4_ nanoparticles was 16.5 ± 1.6 nm in diameter, as measured with transmission electron microscopy. The molar transversal relaxivity was 231 mM^–1^s^–1^. The organic content accounted for ~16.6% of the particles. A room-temperature magnetization curve confirmed that the PEG-coated Fe_3_O_4_ nanocrystals were superparamagnetic, and the particles exhibited a saturation magnetization of 66.0 emu/g, corresponding to 79.1 emu/g Fe_3_O_4_.

The Fe_3_O_4_-Lf conjugate was prepared with the classic EDC/sulfo-NHS-mediated amidation reaction. The hydrodynamic size of PEG-coated Fe_3_O_4_ as determined with dynamic light scattering was 43.6 nm, and this value increased to 48.9 nm after Lf conjugation, suggesting that Lf was effectively coupled to the PEG-coated Fe_3_O_4_ nanoparticles. The polydispersity index of Fe_3_O_4_-Lf (0.386) was similar to that of PEG-coated Fe_3_O_4_ (0.348), indicating that particles did not coagulate during the coupling reaction. The Bradford method was adopted to determine the protein content and revealed ~14.4 Lf molecules per Fe_3_O_4_ nanoparticle on average for the Fe_3_O_4_-Lf. The chemical yield and purity of Fe_3_O_4_-Lf were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=BBB%20and%20delivery%20and%20qiao)]

Qiao et al. first tested the permeability of Fe_3_O_4_-Lf using an in vitro model of the BBB (1). The model was established with primary porcine BCECs that were cultured on microporous filter membrane inserts within a chamber (9, 10). Transendothelial electrical resistance (TEER) was measured after incubation of BCECs with Fe_3_O_4_-Lf or PEG-coated Fe_3_O_4_ at concentrations of 0.04, 0.1, and 0.3 mg Fe/mL, respectively (1). Water was used as a reference for the changes of TEER after nanoparticle exposure. TEER is an indicator of BBB integrity and is usually expressed as measured resistance multiplied by the area of endothelial monolayer (Ω cm^2^). TEER level is mainly determined by the tight junctions between endothelial cells. For the model used by Qiao et al., the TEER was 1,500–2,000 Ω cm^2^, typically >700 Ω cm^2^ after 7 days of culture (1).

At the concentration of 0.04 mg Fe/mL, both Fe_3_O_4_-Lf and PEG-coated Fe_3_O_4_ decreased the TEER level during the initial several hours of exposure. The TEER level recovered over time. Water resulted in similar changes of TEER. These results suggested that the initial decrease of TEER was mainly due to the cell response to the environmental change. However, compared to water, Fe_3_O_4_-Lf led to a lower degree of TEER reduction, while PEG-coated Fe_3_O_4_ resulted in a higher degree of TEER reduction. This trend was more evident at the concentration of 0.1 mg Fe/mL, indicating that the BBB remained more intact in the presence of Fe_3_O_4_-Lf than PEG-coated Fe_3_O_4_. At the high concentration of 0.3 mg Fe/mL, both Fe_3_O_4_-Lf and PEG-coated Fe_3_O_4_ led to much weaker TEER signals than water, suggesting considerable damage to the tight junctions by both Fe_3_O_4_-Lf and PEG-coated Fe_3_O_4_ at this concentration. Overall, the results indicated that Lf could protect the tight junctions from being damaged by the Fe_3_O_4_ nanoparticles at low concentrations. Experiments performed by incubating Lf alone with the BCECs further confirmed that Lf could increase the TEER value.

Qiao et al. then evaluated the efficiency of particle transport by measuring the iron content in the media of the basolateral side after ~18 h incubation of the BCECs with either Fe_3_O_4_-Lf or PEG-coated Fe_3_O_4_ particles (1). At concentrations of 0.04 and 0.1 mg Fe/mL of the agents at the apical side, the transport efficiency of Fe_3_O_4_ particles was strongly enhanced by the Lf conjugation (Table 1). The transport of Fe_3_O_4_-Lf (0.1 mg Fe/mL) could be blocked with Lf, showing that the iron content dropped from 22.0 ± 2.9% to 1.0 ± 0.6% in the presence of 16 times the amount of Lf in the apical media. Consistent with other data, these results also indicate that Lf could facilitate the cross of Fe_3_O_4_ particles through the BBB.

Table 1 Transport efficiency of Fe_3_O_4_-Lf or PEG-coated Fe_3_O_4_ particles in in vitro BBB model.

Agents | Initial Fe concentration at apical side (mg/mL) | Fe content at basolateral side (mg/mL) | Transport efficiency (%)^a^
PEG-Fe_3_O_4_ | 0.04 | 0.0045 ± 0.0003 | 22.5 ± 1.4
Fe_3_O_4_-Lf | 0.04 | 0.0094 ± 0.0028 | 47.0 ± 13.8
PEG-Fe_3_O_4_ | 0.10 | 0.0048 ± 0.0006 | 9.6 ± 1.3
Fe_3_O_4_-Lf | 0.10 | 0.0110 ± 0.0015 | 22.0 ± 2.9

^a^The efficiency was calculated by dividing the feeding amount of Fe by the Fe content in the basolateral medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=BBB%20and%20delivery%20and%20qiao)]

Qiao et al. evaluated the BBB-penetrating efficiency of Fe_3_O_4_-Lf in vivo with T2*-weighted MRI after intravenous injection of PEG-coated Fe_3_O_4_ or Fe_3_O_4_-Lf (10 mg Fe/kg) into Sprague-Dawley rats (n = 2/group) (1). At 15 min after injection, stronger contrast-enhanced vascular images of the brain were obtained with Fe_3_O_4_-Lf than with PEG-coated Fe_3_O_4_. Similarly, a stronger effect on reducing T2* value in the thalamus, brain stem, and frontal cortex was observed at 24 h with Fe_3_O_4_-Lf than with PEG-coated Fe_3_O_4_. These results supported the conclusion that the BBB-penetrating efficiency of Fe_3_O_4_ particles could be enhanced through Lf-receptor-mediated transport in vivo.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Qiao R., Jia Q., Huwel S., Xia R., Liu T., Gao F., Galla H.J., Gao M. (2012). Receptor-mediated delivery of magnetic nanoparticles across the blood-brain barrier. ACS Nano.
2 Fortin D. (2012). The blood-brain barrier: its influence in the treatment of brain tumors metastases. Curr Cancer Drug Targets.
3 Fu B.M. (2012). Experimental methods and transport models for drug delivery across the blood-brain barrier. Curr Pharm Biotechnol.
4 Huang R., Ke W., Han L., Liu Y., Shao K., Jiang C., Pei Y. (2010). Lactoferrin-modified nanoparticles could mediate efficient gene delivery to the brain in vivo. Brain Res Bull.
5 Huang R.Q., Ke W.L., Qu Y.H., Zhu J.H., Pei Y.Y., Jiang C. (2007). Characterization of lactoferrin receptor in brain endothelial capillary cells and mouse brain. J Biomed Sci.
6 Suzuki Y.A., Lopez V., Lonnerdal B. (2005). Mammalian lactoferrin receptors: structure and function. Cell Mol Life Sci.
7 Fillebeen C., Descamps L., Dehouck M.P., Fenart L., Benaissa M., Spik G., Cecchelli R., Pierce A. (1999). Receptor-mediated transcytosis of lactoferrin through the blood-brain barrier. J Biol Chem.
8 Xie H., Zhu Y., Jiang W., Zhou Q., Yang H., Gu N., Zhang Y., Xu H., Yang X. (2011). Lactoferrin-conjugated superparamagnetic iron oxide nanoparticles as a specific MRI contrast agent for detection of brain glioma in vivo. Biomaterials.
9 Garcia-Garcia E., Gil S., Andrieux K., Desmaele D., Nicolas V., Taran F., Georgin D., Andreux J.P., Roux F., Couvreur P. (2005). A relevant in vitro rat model for the evaluation of blood-brain barrier translocation of nanoparticles. Cell Mol Life Sci.
10 Roux F. (2005). andCouraud, P.O. Rat brain endothelial cell lines for the study of blood-brain barrier permeability and transport functions. Cell Mol Neurobiol.